# ^131^I-NP-4 anti-CEA monoclonal antibody

Chemical name: | ^131^I-NP-4 anti-CEA monoclonal antibody
Abbreviated name: | ^131^I-NP-4 MAb
Synonym:
Agent Category: | Antibody
Target: | Carcinoembryonic antigen (CEA)
Target Category: | Antibody to antigen binding
Method of detection: | Single Photon Emission Computed Tomography (SPECT), planar gamma imaging
Source of signal /contrast: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=180211), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=29856) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5670) for more information about CEA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28131I-NP-4%20MoAb%20OR%20I-131-NP-4%20MoAb%20OR%20radioiodinated%20NP-4%20monoclonal%20antibody%20OR%20131I-NP-4%20IgG%29)]

^131^I-NP4 MAb, which is formed by the conjugation of ^131^I with an intact murine anti-carcinoembryonic antigen (CEA) monoclonal antibody (MAb), can be used for imaging and therapy of CEA- expressing cancers (1, 2). ^131^I has a physical t_½_ of 8 days.

CEA was first identified from extracts of human adenocarcinoma of the colon (3). It is a β-glycoprotein, and its predominant expression on the cell surface is increased in a variety of carcinomas, particularly of the gastrointestinal tract, as well as in fetal gastrointestinal tissues and in certain inflammatory states, such as inflammatory bowel disease (4, 5). CEA, which exhibits extensive heterogeneity in its physicochemical and immunologic properties (2, 3), has a molecular weight of 200 kDa and can be shed and detected in the serum (2). It has been used as a serum marker for monitoring disease status in patients who have various CEA- secreting tumors (gastrointestinal, lung, medullary, thyroid, uterine, ovarian, and bladder carcinomas). Other cross-reactive, but genetically distinct, CEA variants have been identified, including nonspecific cross-reactive antigen (NCA) and meconium antigen (MA) (6).

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (4). Primus et al. (2) studied the immunologic heterogeneity of CEA by use of four MAbs to differentiate the antigenic sites on colonic cancer CEA. They classified the MAbs into three general classes based on their reactivity with CEA, NCA, and MA. The class I antibody, NP-1, had high affinity for CEA and MA but low affinity for NCA. The class II antibodies, NP-2 and NP-3, had moderate affinities for CEA and MA. The class III antibody, NP-4, appeared to recognize determinants unique to CEA and had no affinity for NCA or MA. Because of this specificity, NP-4 MAb in the form of intact IgG has been labeled with radioisotopes for CEA tumor imaging and therapy (7). NP-4 MAb is covalently linked to ^131^I by radioiodination with Na^131^I. ^131^I emits both gamma and beta radiation, and it can be used for imaging at low doses and for therapy at high doses. NP-4 MAb in the form of Fab’ fragment has also been labeled with ^99m^Tc for imaging (8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28131I-NP-4%20MoAb%20OR%20I-131-NP-4%20MoAb%20OR%20radioiodinated%20NP-4%20monoclonal%20antibody%20OR%20131I-NP-4%20IgG%29%29%20AND%20synthesis)]

NP-4 MAb is an IgG_1_ subtype and has a CEA affinity in the range of 10^8^ M^−1^ (2). NP-4 MAb was initially produced by Primus et al. (5, 9) in 1983 with the use of the hybridoma technique and CEA isolated from liver metastases of a colonic adenocarcinoma. The NP-4 MAb was produced in mice and purified from ascites fluid by protein A and ion-exchange column chromatography at 4 ^o^C (10). The final purity and identity were confirmed by immunoelectrophoresis, sodium dodecyl sulfate (SDS) gel electrophoresis, and size-exclusion high-performance liquid chromatography (HPLC). Direct radioiodination of the intact whole MAb with ^131^I was performed by the chloramines-T or IodoGen method. The specific activity obtained was 444-592 MBq/mg (12-16 mCi/mg), or 67.3-89.7 GBq/µmol (1.8-2.4 Ci/µmol) based on a molecular weight of 150,000 for the MAb. in 1983 with the use of the hybridoma technique and CEA isolated from liver metastases of a colonic adenocarcinoma). The radioimmunoreactivity was >70% based on binding of ^131^I-NP-4 MAb to a CEA-immunoadsorbent column. The radiochemical purity was >95%, and 85-95% of the radioactivity was native-size IgG as determined by size-exclusion HPLC.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28131I-NP-4%20MoAb%20OR%20I-131-NP-4%20MoAb%20OR%20radioiodinated%20NP-4%20monoclonal%20antibody%20OR%20131I-NP-4%20IgG%29%20AND%20in%20vitro)]

Primus et al.(2) first reported the production of NP-4 anti-CEA MAb. Using a competitive radioimmunoassay method, they obtained an affinity constant (K) for CEA of 8.9 х 10^8^ M^−1^. NP-4 MAb did not appear to bind to NCA or MA.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28131I-NP-4%20MoAb%20OR%20I-131-NP-4%20MoAb%20OR%20radioiodinated%20NP-4%20monoclonal%20antibody%20OR%20131I-NP-4%20IgG%29%20AND%20rodentia)]

Sharkey et al.(11) studied the biodistribution of ^131^I-NP-4 MAb in nude mice bearing the CEA-producing human colorectal cancer, GW-39. NP-4 MAb was radiolabeled at a ratio of 0.06 mg MAb/mCi to achieve a specific activity of 370-518 MBq (10-14 mCi)/mg (56.1-78.5 GBq (1.5-2.1 Ci)/µmol). Maximum tumor localization of ^131^I-NP-4 MAb occurred within 3 days and reached about 30% injected dose (ID)/g. The tumor radioactivity decreased between days 7 and 14. The tumor/nontumor tissue ratios on day 1 for the kidney, liver, lung, spleen, and blood were 2.5 ± 0.9, 3.8 ± 1.3, 2.1 ± 0.8, 4.8 ± 2.2, and 0.9 ± 0.3, respectively. By day 14, these ratios increased to 50.0 ± 20.0, 59.0 ± 21.3, 36.2 ± 13.0, 101.0 ± 57.0, and16.6 ± 7.0,

Boerman et al. (12) studied the influence of antibody protein dose on the biodistribution of ^131^I-NP-4 MAb in small GW-39 tumors (0.1-0.4 g) implanted in nude mice. NP-4 MAb was labeled with ^131^I by the chloramine-T method with a specific activity of 444-555 MBq (12-15 mCi)/mg (67.3-84.1 GBq (1.8-2.3 Ci)/µmol). Increasing amounts of unlabeled antibody were added to 1 µg of ^131^I-NP-4 MAb preparations to achieve 5 different protein doses. Seven days after injection, tumor radioactivity of ^131^I-NP-4 MAb remained constant up to an antibody protein dose of 100 µg/animal. The tumor radioactivities (in %ID/g) were 20.4 ± 1.9, 27.1 ± 9.3, 25.0 ± 4.2, 11.4 ± 0.2, and 7.2 ± 1.6 for protein doses of 1, 10, 100, 500, and 1000 µg/animal, respectively. In comparison, the radioactivities in the normal tissues were not decreased at higher protein doses.

Blumenthal et al. (13) evaluated the localization of ^125^I-NP-4 MAb in 4 size-matched human colonic carcinomas (LSi74T, GW-39, GS-2, and Moser) of varying histopathology grown s.c. in nude mice. They found that, unless serum CEA levels became very high (>150 ng/ml), ^125^I-NP-4 MAb did not complex with circulating CEA. Differences in tumor vascularity did not appear to have a strong influence on the antibody tumor localization. Intra-tumoral distribution of antigen and subcellular accessibility of antigen for radiolabeled antibody appeared to have a bigger influence. Low ^125^I-NP-4 MAb targeting was found in tumors with 90% CEA within the tumor cells and slow ^125^I-NP-4 MAb internalization.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28I-131-NP-4%20MoAb%20OR%20radioiodinated%20NP-4%20monoclonal%20antibody%20OR%20131I-NP-4%20IgG%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Sharkey et al. (14) studied the biodistribution of ^131^I-NP-4 MAb in hamsters bearing the GW-39 tumor. NP MAbs (NP-2, NP-3, and NP-4) were radioiodinated with ^131^I by the chloramines-T method to achieve a specificity activity of 444-555 MBq (12-15 mCi)/mg (67.3-84.1 GBq (1.8-2.3 Ci)/µmol). An irrelevant mouse myeloma IgG (Ag8) labeled with ^125^I was also used to indicate the nonspecific localization of a MAb. Each tumor bearing hamster received intracardiac injections containing 5550-7400 kBq (150-200 µCi)/10-15 µg of ^131^I-labeled antibody and 1850 kBq (50 µCi)/5 µg of ^125^I-Ag8. A tumor localization index was calculated from the ratio of specific versus irrelevant antibody in the tumor divided by the ratio of specific versus irrelevant antibody in the blood. All ^131^I-labeled NP MAbs showed a preferential localization for GW-39 compared with ^125^I-Ag8. The tumor radioactivities (%ID/g) for ^131^I-NP-4 MAb (n = 5) were 1.3 ± 0.09, 1.0 ± 0.06, and 0.7 ± 0.04 on days 1, 3, and 7 after injection, respectively. The tumor localization indices were 0.9-1.5, 2-2.5, and 3.5-4.5 on days 1, 3, and 7, respectively. The tumor/blood, tumor/liver, tumor/spleen, tumor/kidney, and tumor/lung ratios of ^131^I-NP-4 MAb on day 7 were 1.60 ± 0.16, 6.5 ± 0.6, 7.1 ± 0.6, 5.1 ± 0.5, and 3.9 ± 0.4, respectively.

Wahl et al. (5) performed imaging of s.c. GW-39 bearing Syrian hamsters. Doses containing 1850 kBq (50 µCi)/14 µg of ^131^I-NP-4 MAb were given by intracardiac injection. One to 2 days after injection, the tumor was visible. By 6 days, there was a gradual decrease in background activity with preservation of most radioactivity in the tumor. After 7 days, the organ radioactivities in %ID/g for the tumor, blood, liver, kidney, spleen, and lung (n = 4 for each) were 1.21 ± 0.14, 0.75 ± 0.12, 0.16 ± 0.02, 0.17 ± 0.03, 0.18 ± 0.02, and 0.26 ± 0.04, respectively. A specific localization ratio (ratio of ^131^I-NP-4 MAb %ID/g to a nonspecific MAb %ID/g) based on the localization of a nonspecific ^125^I-MOPC MAb in the same animal was calculated as 1.97 ± 0.125 for the tumor at 7 days after injection. On day 11, the total radioactivity left in the tumor was 8.87 ± 1.38% ID, about 63% of the whole-body radioactivity.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28131I-NP-4%20MoAb%20OR%20I-131-NP-4%20MoAb%20OR%20radioiodinated%20NP-4%20monoclonal%20antibody%20OR%20131I-NP-4%20IgG%29%20AND%20%28primate%20NOT%20human%29)]

Losman et al. (15) immunized a baboon with NP-4 MAb to produce anti-NP-4 antibody. This baboon antibody inhibited specifically the binding between NP-4 and CEA in enzyme-linked immunosorbent assay (ELISA). Mice immunized with this baboon anti-idiotype antibody produced antibody to the CEA epitope recognized by NP-4 MAb. The study suggested that baboon anti-idiotype antibodies functionally mimic a CEA epitope.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28131I-NP-4%20MoAb%20OR%20I-131-NP-4%20MoAb%20OR%20radioiodinated%20NP-4%20monoclonal%20antibody%20OR%20131I-NP-4%20IgG%29%20AND%20human)]

The immunologic, pharmacokinetic, and targeting properties of ^131^I-NP-4 MAb were studied in patients with colorectal carcinoma (7). NP-4 MAb was radiolabeled with ^131^I by the chloramine-T method. Radiolabeling efficiencies were >70% with a specific activity of 444-666 MBq (12-18 mCi)/mg (67.3-100.9 GBq (1.8-2.7 Ci)/µmol). Immunoreactivities were typically 80-90%. Patients were given 92.5-185 MBq (2.5-5 mCi) of ^131^I-NP-4 MAb in less than 1 mg for imaging. The blood clearance of ^131^I-NP-4 MAb had an elimination t_½_ of 29 ± 14 h. For additional patients who received protein doses of >1 mg, the blood clearance was prolonged. Most patients had less than 20% complexing with CEA at 1 or 24 h after injection. The sensitivity, specificity, and accuracy of detecting tumor sites in 21 patients were 73.5%, 88.6%, and 81.2%, respectively. Losman et al. (16) produced anti-idiotype antibody from a cancer patient treated with^131^I-NP-4 and suggested that human anti-idiotype antibody to NP-4 could antigenically mimic the CEA epitope recognized by NP-4. Murray et al. (17) compared the tumor localization of ^125^I-NP-4 MAb (whole antibody) with its ^131^I-NP-4 MAb F(ab´)_2_ fragment in 5 patients with colorectal cancer. All 5 patients received a combination of 74 MBq (2 mCi)/1 mg of ^125^I-NP-4 MAb and 370 MBq (10 mCi)/1 mg of ^131^I-NP-4 MAb F(ab´)_2_ fragment. The tumor radioactivities (%ID/g) for ^125^I-NP-4 MAb and ^131^I-NP-4 MAb F(ab´)_2_ fragment were 2.6 ± 0.94 and 2.0 ± 0.57, respectively. The plasma t_½_ (h) and 48-h urinary excretion rates (%) for ^131^I-NP-4 MAb F(ab’)_2_ and ^125^I-NP-4 MAb were 29 ± 3.2 h and 50.2 ± 5%, and 43.2 ± 7.3 h, and 56.7 ± 4.7%, respectively.

In a phase I/II clinical trial of ^131^I-NP-4 MAb, 57 patients with CEA-expressing tumors (29 colorectal, 9 lung, 7 pancreas, 6 breast, and 4 medullary thyroid cancer) in advanced metastatic stages were studied (1). Patients received 296-1110 MBq (8-30 mCi)/1-3 mg ^131^I-NP-4 MAb with a specific activity of 444-592 MBq (12-16 mCi)/mg (67.3-89.7 GBq (1.8-2.4 Ci)/µmol) for planar and single-photon emission computed tomography (SPECT) imaging. Thirty-seven patients had already received murine MAbs before the study. Ten patients had HAMA titers >300 units. Above this titer, rapidly increasing plasma and whole-body clearance rates were observed. Colorectal cancer patients had a faster blood t_½_ (21.4 ± 11.1 h) and whole-body t_½_ (61.9 ± 39.9 h) than patients with other types of cancers. In the presence of human anti-mouse antibodies (HAMAs), ^131^I-NP-4 MAb was increasingly localized in the liver, spleen, and bone marrow as high-molecular-weight fractions at 1 h (determined by size-exclusion chromatography). At 24 h, the majority of ^131^I-NP-4 MAb was rapidly excreted renally as low-molecular-weight fractions (metabolites). No significant difference in pharmacokinetics was observed between HAMA-negative patients and patients with HAMA titers as long as HAMA titers were <300 units. The red marrow and whole-body radiation absorbed doses in HAMA-negative (<300 units) patients were 2.2 cGy/mCi and 0.73 ± 0.37 cGy/mCi, respectively. The highest absorbed dose (26.06 ± 20.83 cGy/mCi) was to the (blocked) thyroid. The kidney and spleen received the second highest doses of 3.57 ± 0.97 cGy/mCi and 3.57 ± 1.48 cGy/mCi, respectively. In the same clinical trial, the therapeutic efficacy of ^131^I-NP-4 MAb for treating CEA-expressing tumors was studied, and it was found that the red marrow was the dose-limiting organ. Mittal et al. (18), in a study involving 9 patients, showed that it was feasible to combine hyperthermia and ^131^I-NP-4 MAb for treating patients who had colorectal carcinoma with liver metastases.

## NIH Support

NCI CA39841, CA-37895, NIH S07 RR05903-04, NCI CA23154, CA24376, CA54425, CA66906, CA 67026, NCI CA-10815, CA-33491, CA-21124.

## References

1 Behr T.M., Sharkey R.M., Juweid M.E., Dunn R.M., Vagg R.C., Ying Z., Zhang C.H., Swayne L.C., Vardi Y., Siegel J.A., Goldenberg D.M. (1997). Phase I/II clinical radioimmunotherapy with an iodine-131-labeled anti-carcinoembryonic antigen murine monoclonal antibody IgG. J Nucl Med.
2 Primus F.J., Freeman J.W., Goldenberg D.M. (1983). Immunological heterogeneity of carcinoembryonic antigen: purification from meconium of an antigen related to carcinoembryonic antigen. Cancer Res.
3 Gold P., Freedman S.O. (1964). Demonstration of tumor-specific antigens in human colonic carcinomata by immunological tolerance and absorption techniques. The Journal of Experimental Medicine.
4 Kowalsky, R.J., and S.W. Falen, Radiopharmaceuticals in nuclear pharmacy and nuclear medicine. 2004, American Pharmacists Association: Washington, D.C. p. 733-752.
5 Wahl R.L., Philpott G., Parker C.W. (1983). Monoclonal antibody radioimmunodetection of human-derived colon cancer. Invest Radiol.
6 Package Insert. CEA-Scan (Arcitumomab) for the preparation of Tc 99m Arcitumomab. 1999, Immunomedics, Inc. p. 1-15.
7 Sharkey R.M., Goldenberg D.M., Goldenberg H., Lee R.E., Ballance C., Pawlyk D., Varga D., Hansen H.J. (1990). Murine monoclonal antibodies against carcinoembryonic antigen: immunological, pharmacokinetic, and targeting properties in humans. Cancer Res.
8 Wegener W.A., Petrelli N., Serafini A., Goldenberg D.M. (2000). Safety and efficacy of arcitumomab imaging in colorectal cancer after repeated administration. J Nucl Med.
9 Kohler G., Milstein C. (1975). Continuous cultures of fused cells secreting antibody of predefined specificity. Nature.
10 Behr T.M., Goldenberg D.M., Scheele J.R., Wolf F.G., Becker W. (1997). Clinical relevance of immunoscintigraphy with 99mTc-labelled anti-CEA antigen-binding fragments in the follow-up of patients with colorectal carcinoma. Assessment of surgical resectability with a combination of conventional imaging methods. Dtsch Med Wochenschr.
11 Sharkey R.M., Gold D.V., Aninipot R., Vagg R., Ballance C., Newman E.S., Ostella F., Hansen H.J., Goldenberg D.M. (1990). Comparison of tumor targeting in nude mice by murine monoclonal antibodies directed against different human colorectal cancer antigens. Cancer Res.
12 Boerman O.C., Sharkey R.M., Wong G.Y., Blumenthal R.D., Aninipot R.L., Goldenberg D.M. (1992). Influence of antibody protein dose on therapeutic efficacy of radioiodinated antibodies in nude mice bearing GW-39 human tumor. Cancer Immunol Immunother.
13 Blumenthal R.D., Sharkey R.M., Kashi R., Natale A.M., Goldenberg D.M. (1992). Physiological factors influencing radioantibody uptake: a study of four human colonic carcinomas. Int J Cancer.
14 Sharkey R.M., Primus F.J., Shochat D., Goldenberg D. M. (1988). Comparison of tumor targeting of mouse monoclonal and goat polyclonal antibodies to carcinoembryonic antigen in the GW-39 human tumor-hamster host model. Cancer Research.
15 Losman M.J., Monestier M., Hansen H.J., Goldenberg D.M. (1990). Baboon anti-idiotype antibodies mimic a carcinoembryonic antigen epitope. Int J Cancer.
16 Losman M.J., Hansen H.J., Sharkey R.M., Goldenberg D.M., Monestier M. (1991). Human response against NP-4, a mouse antibody to carcinoembryonic antigen: human anti-idiotype antibodies mimic an epitope on the tumor antigen. Proc Natl Acad Sci U S A.
17 Murray J.L., Rosenblum M.G., Zhang H.Z., Podoloff D.A., Kasi L.P., Curley S.A., Chan J.C., Roh M., Hohn D.C., Brewer H., Cunningham J.E., Thompson L.B., Bhadkamkar M.S., Pinsky C.M., Fogler W.E. (1994). Comparative tumor localization of whole immunoglobulin G anticarcinoembryonic antigen monoclonal antibodies IMMU-4 and IMMU-4 F(ab')2 in colorectal cancer patients. Cancer.
18 Mittal B.B., Zimmer M.A., Sathiaseelan V., Benson A.B., Mittal R.R., Dutta S., Rosen S.T., Spies S.M., Mettler J.M., Groch M.W. (1996). Phase I/II trial of combined 131I anti-CEA monoclonal antibody and hyperthermia in patients with advanced colorectal adenocarcinoma. Cancer.